# ^111^In-Labeled DOTA-conjugated 6-aminohexanoic linker-containing variant of anti-epidermal growth factor receptor 2 Affibody Z_HER2:342_ (ABY-003)

Chemical name: | ^111^In-Labeled DOTA-conjugated 6-aminohexanoic linker-containing variant of anti-epidermal growth factor receptor 2 Affibody Z_HER2:342_ (ABY-003)
Abbreviated name: | [^111^In]-ABY-003
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibody&cmd=DetailsSearch)]

An Affibody molecule is a chain of 58 amino acids (~6.5 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained through chemical synthesis or produced in bacteria with the use of recombinant technology (1). Because of their small size and high chemical and thermal stability, these molecules are used as radiolabeled probes for the targeted detection and treatment of malignant tumors as discussed elsewhere (1-3).

The epidermal growth factor receptor 2 (HER2) is considered to be an important Affibody target because it is believed to promote the development of the malignant phenotype, it plays a role in the development of resistance to anticancer drugs and radiation therapy, it is overexpressed in several different cancer tumor cells, and it often indicates a poor prognosis for the patient (4). Several radionuclide-labeled Affibodies and their derivatives, such as Z_HER2:342_, have been evaluated to detect tumors expressing HER2 in preclinical studies as discussed by Tolmachev (5). Earlier, a derivative of the Z_HER2:342_ Affibody, designated ABY-002, which has the radiometal chelator 1,4,7,10-tetraazacyclododecane-N,N',N,N'-tetraacetic acid (DOTA) linked directly to the N-terminal valine of the molecule was constructed, radiolabeled with ^111^In or ^68^Ga, and evaluated for the imaging of malignant tumors that express HER2 (6). Although radiolabeled ABY-002 (both with ^111^In or ^68^Ga) could detect these tumors under in vivo conditions, the Z_HER2:342_ Affibody derivative exhibited a reduced affinity for HER2 (K_D_ = 65 pM) compared to the parent Affibody (K_D_ = 22 pM).

From this study, it was concluded that the reduced affinity of ABY-002 for the receptor is probably due to a steric hindrance from the DOTA moiety, which is located very close to the HER2 binding site of the molecule. Tolmachev et al. decided to introduce a linker between the DOTA moiety and the HER2 binding sequence and evaluate whether this modification reduced or abolished the steric obstruction that may reduce the affinity of the Affibody for the receptor (7). The investigators placed an aliphatic linker (6-aminohexanoic acid) between DOTA and the valine on the N-terminal of ABY-002, labeled the modified Affibody (ABY-003) with ^111^In ([^111^In]-ABY-003), and evaluated the biodistribution and tumor detection properties of [^111^In]-ABY-003 in mice bearing HER2-expressing LS174T cell xenograft tumors (a human colon adenocarcinoma cell line showing a moderate expression level of HER2) or SKOV-3 cell xenograft tumors (a human ovarian carcinoma cell line showing a high expression level of HER2) (7).

### Related Resource Links

Affibody-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Other epidermal growth factor receptor (EGFR) imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man)

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR

Anti-EGFR antibody clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies)

EGFR pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) in Pathways Interaction Database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ABY-003%20synthesis&cmd=DetailsSearch)]

The synthesis and ^111^In labeling of the ABY-003 Affibody have been described by Tolmachev et al. (7). The radiochemical yield of [^111^In]-ABY-003 was 98.9 ± 0.9% (n = 22 synthesis procedures), and the final product was used in all experiments without further purification. The specific activity of the labeled Affibody was reported to be up to 14 GBq/μmol (0.476 mCi/μmol).

In some studies, ^111^In-labeled ABY-002 ([^111^In]-ABY-002) was used for comparison purposes (7). The labeling of ABY-002 was performed in the same manner as for ABY-003. The radiochemical purity, radiochemical yield, and specific activity of [^111^In]-ABY-002 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ABY-003%20in%20vitro&cmd=DetailsSearch)]

The in vitro stability of [^111^In]-ABY-003 was tested by incubating the labeled Affibody with or without 500-fold molar excess ethylenediamine acetic acid (EDTA) in phosphate-buffered saline for 6 h at room temperature (7). At the end of incubation, instant thin-layer chromatography analysis showed that 97.6 ± 0.2% of ^111^In remained associated with the Affibody in the test samples (with EDTA) versus 99.6 ± 0.3% in the controls (without EDTA), indicating that the [^111^In]-ABY-003 had high stability at room temperature.

The binding of ABY-003 to the extracellular domain of HER2 (HER2-ECD) and to the chimeric HER2/Fc fusion protein (HER2/Fc; has the HER2-ECD fused to the Fc region of human IgG (8)) was determined with the Biacore technique and compared with the binding of ABY-002 and ABY-004, the unmodified parent molecule of ABY-002 (7). The K_D_ values of ABY-004, ABY-002, and ABY-003 for HER2-ECD were reported to be 45 ± 11 pM, 118 ± 5 pM, and 135 ± 3 pM, respectively. With HER2/Fc, these values were 58 ± 2 pM, 139 ± 8 pM, and 145 ± 5 pM for ABY-004, ABY-002, and ABY-003, respectively.

The in vitro HER2 binding specificity of [^111^In]-ABY-003 was tested by exposing SKOV-3 cells (~1.2 × 10^6^ HER2 receptors/cell) to the labeled Affibody (1 nM) for 1 h at 37°C (7). Under these conditions, 43 ± 2% of the radioactivity remained associated with the cells at the end of the incubation period. When the cells were preincubated with excess unlabeled His_6_-Z_HER2:342_ (concentration not reported), which is another HER2-binding derivative of the Z_HER2:342_ Affibody, the amount of radioactivity that remained associated with the cells was reduced to 0.12 ± 0.05% (P < 0.0001). This indicated that [^111^In]-ABY-003 bound specifically to the HER2 on the cells.

A cell internalization study with [^111^In]-ABY-003 revealed that 37.9 ± 0.2% of radioactivity was taken up by the cells after 24 h at 37°C (7). This rate of internalization was similar to that observed with [^111^In]-ABY-002 (9). This indicated that placement of the aliphatic linker between the DOTA and the Z_HER2:342_ Affibody did not affect the cellular internalization of the Affibody.

After an interrupted incubation, the retention of [^111^In]-ABY-003 by SKOV-3 cells was 84.8 ± 0.0% and 69.2 ± 0.3% at 24 h and 72 h, respectively, versus retention levels of 90.0 ± 0.6% and 79.1 ± 0.4% for [^111^In]-ABY-002 at the same time points (7). This indicated that the cellular retention of [^111^In]-ABY-002 was slightly superior to that of its derivative.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-003%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-ABY-003 was compared with that of [^111^In]-ABY-002 in normal Naval Medical Research Institute mice (7). The animals (n = 4 mice/group) were subcutaneously injected with a total of 1 μg protein adjusted with an appropriate amount of unlabeled Affibody (specific activity, 213 MBg/μmol (5.75 mCi/μmol)), and the mice were euthanized at predetermined time points ranging from 1 h to 24 h postinjection (p.i.) to determine radioactivity content of the various tissues. Both labeled Affibodies were cleared rapidly from the blood circulation and whole body of the animals. Although there was low accumulation of radioactivity in the liver with both radiolabeled Affibodies, accumulation of label from [^111^In]-ABY-003 was observed in this organ at all the time points to be significantly higher (P < 0.05) than that of [^111^In]-ABY-002. Except for the kidneys, the accumulation of radioactivity was low in the different organs with both labeled Affibodies. This study indicated that [^111^In]-ABY-003 had a biodistribution pattern similar to that of the parent Affibody (ABY-002) in rodents.

In another study, the biodistribution of [^111^In]-ABY-003 was studied at 4 h p.i. as described above in mice (n = 4 animals/group) bearing LS174T cell xenograft tumors (7). The biodistribution pattern of radioactivity in the various organs of these mice was similar to that observed with the NMRI mice as detailed above. The tumor showed an accumulation of 9.1 ± 0.5% injected dose per gram tissue (% ID/g). With [^111^In]-ABY-003, the tumor/blood, tumor/liver, and tumor/muscle ratios were 18 ± 4, 6 ± 1, and 70 ± 36, respectively. The uptake of radioactivity in tumors of mice pretreated with excess unlabeled Z_HER2:342_ Affibody (~6.6 nM) was 0.5 ± 0.2% ID/g (P <0.000%), indicating that [^111^In]-ABY-003 bound specifically to the HER2-expressing tumors.

The biodistribution of [^111^In]-ABY-003 was also investigated in mice bearing SKOV-3 cell xenograft tumors (n = 4 animals/group), and data obtained from this study were compared to data obtained from a similar study performed with [^111^In]-ABY-002 (7). Both labeled Affibodies showed a similar biodistribution pattern in the animals. The only difference was that the SKOV-3 cell tumors showed a higher accumulation of radioactivity from [^111^In]-ABY-003 (14 ± 2% ID/g) than did the LS174T lesions (9.1 ± 0.5% ID/g; see above). At 4 h p.i., the tumor/heart, tumor/lung, tumor/liver, tumor/spleen, and tumor/muscle ratios were 48 ± 16, 26 ± 3, 9 ± 1, 31 ± 6, and 110 ± 40, respectively, which were higher than the ratios obtained with [^111^In]-ABY-002. For details, see Table 4 in Tolmachev et al. (7).

Mice bearing SKOV-3 cell tumors (n = 3 animals) were injected with [^111^In]-ABY-003 to acquire whole-body gamma planar images at 4 h p.i (7). The xenograft lesions and the kidneys were clearly visible in the images, but the other organs were not visualized. Therefore, high-contrast images of tumors expressing HER2 were generated with the labeled ABY-003 Affibody.

From these studies, the investigators concluded that the introduction of a linker between the metal chelator and the N-terminus of the Z_HER2:342_ Affibody had little influence on the biological properties of the molecule (7). The rapid clearance of [^111^In]-ABY-003 from the blood and whole body of the mice resulted in a higher tumor/organ ratio of radioactivity, although in general, compared to [^111^In]-ABY-002, a lower accumulation of label was observed in the various with [^111^In]-ABY-003.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-003%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-003%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-ABY-003%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
2 Lofblom J., Feldwisch J., Tolmachev V., Carlsson J., Stahl S., Frejd F.Y. (2010). Affibody molecules: engineered proteins for therapeutic, diagnostic and biotechnological applications. FEBS Lett.
3 Tolmachev V., Orlova A. (2010). Influence of labelling methods on biodistribution and imaging properties of radiolabelled peptides for visualisation of molecular therapeutic targets. Curr Med Chem.
4 Capala J., Bouchelouche K. (2010). Molecular imaging of HER2-positive breast cancer: a step toward an individualized 'image and treat' strategy. Curr Opin Oncol.
5 Tolmachev V. (2008). Imaging of HER-2 overexpression in tumors for guiding therapy. Curr Pharm Des.
6 Tolmachev V., Velikyan I., Sandstrom M., Orlova A. (2010). A HER2-binding Affibody molecule labelled with 68Ga for PET imaging: direct in vivo comparison with the 111In-labelled analogue. Eur J Nucl Med Mol Imaging.
7 Tolmachev V., Feldwisch J., Lindborg M., Baastrup B., Sandstrom M., Orlova A. (2011). Influence of an aliphatic linker between DOTA and synthetic Z(HER2:342) Affibody molecule on targeting properties of the (111)In-labeled conjugate. Nucl Med Biol.
8 Orlova A., Tolmachev V., Pehrson R., Lindborg M., Tran T., Sandstrom M., Nilsson F.Y., Wennborg A., Abrahmsen L., Feldwisch J. (2007). Synthetic affibody molecules: a novel class of affinity ligands for molecular imaging of HER2-expressing malignant tumors. Cancer Res.
9 Wallberg H., Orlova A. (2008). Slow internalization of anti-HER2 synthetic affibody monomer 111In-DOTA-ZHER2:342-pep2: implications for development of labeled tracers. Cancer Biother Radiopharm.